# ^99m^Tc-N_2_S_2_-Tat(49-57)-Lys^3^-bombesin

Chemical name: | ^99m^Tc-N_2_S_2_-Tat(49-57)-Lys^3^-bombesin
Abbreviated name: | ^99m^Tc-Tat-BN
Synonym:
Agent Category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=4885361), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=61677286) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2925) for more information about gastrin-releasing peptide receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22bombesin%22%25GRPR%20imaging)]

^99m^Tc-N_2_S_2_-Tat(49-57)-Lys^3^-bombesin (^99m^Tc-Tat-BN) is a hybrid peptide synthesized and labeled with ^99m^Tc by Santos-Cuevas et al. for molecular imaging of tumors expressing gastrin-releasing peptide receptor (GRPR) (1).

Bombesin (BN) is an amphibian neuropeptide consisting of 14 amino acids (pGlu-Gln-Arg-Leu-Gly-Asn-Gln-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_) (2, 3), first isolated from frog skin in 1970 (4). The search for its mammalian counterpart led to the discovery of gastrin-releasing peptide (GRP), which consists of 27 amino acids. GRP and BN share an identical C-terminal region (-Trp-Ala-Val-Gly-His-Leu-Met-NH_2_), which is necessary for receptor binding and signal transduction (5, 6). Besides the release of gastrin, GRP and BN-like peptides also produce a wide range of other biological responses in diverse tissues such as secretion of endocrine and exocrine glands, maintenance of circadian rhythm, regulation of satiety, and contraction of smooth muscles (7). They also act as potential growth factors for both normal and cancer cells (3, 5, 6). There are four members of the BN receptor family, including three mammalian receptors: GRPR (BB_2_ or BRS2; 384 amino acids), neuromedin B receptor (NMBR, BB_1_, or BRS1; 390 amino acids), and BN-like receptor 3 (BB_3_, BRS3, or orphan; 399 amino acids) (5, 7, 8); the fourth receptor (BB_4_) has only been found in amphibians. GRPR is the only well characterized receptor of this family. GRPR is a glycosylated, 7-transmembrane, G-protein–coupled receptor that, upon binding with its ligands, gives rise to a complex cascade of intracellular reactions. It is normally found in non-neuroendocrine tissues of the breast and pancreas and in neuroendocrine cells of the brain, gastrointestinal tract, lung, and prostate (9). Interestingly, GRPR is overexpressed in prostate cancer as well as tumors of breast, lung, pancreas, ovary, kidney, and gastrointestinal tract. It has been reported that GRPR is expressed at a high density in the intraepithelial neoplasia and primary carcinoma of prostate, whereas normal prostate tissue and, in most cases, benign prostate hyperplasia are predominantly GRPR-negative (10-13).

GRPR has attracted significant interest as a target for tumor detection, tumor staging, and evaluation of tumor response to therapy (5, 6, 8, 11). A large number of BN derivatives have been developed, and they have been labeled with ^99m^Tc, ^177^Lu, ^67^Ga, and ^111^In for single-photon emission computed tomography and with ^64^Cu, ^68^Ga, and ^18^F for positron emission tomography. The published BN derivatives can be generally classified as truncated BN (6–14 or 7–14) or full-length BN (1-14) analogs (1, 10, 12-17). The truncated BN analogs seem to be favorable because they are usually more stable than the full-length tetradecapeptides for in vivo applications, and they still bind to the GRPR adequately. However, the full-length peptides offer different labeling methods by attachment of functional groups to the amino acid 1 to 6. In many cases, the amino acids on position 13 (Leu) and 14 (Met) have been replaced by unnatural amino acids (cyclohexylalanine (CyHAla) and norleucine (Nle)), and Lys has been placed on position 3 for attachment of radiolabels with reactive esters. Spacers, chelators, or radiometals have also been widely used for conjugation and for favorable kinetics (18). The BN derivatives can also be divided into agonists and antagonists (19-21). By far, most BN derivatives are agonists. Agonists are internalized into and accumulate within cells, and they have been assumed to exhibit higher uptake by cancer cells than antagonists. However, some reports have shown that uptake of antagonists is much higher than that of agonists because antagonists may have stronger binding for the GRPR than agonists (19, 20).

An optimal BN-like radiotracer needs to meet several requirements: high affinity for GRPR, with rapid and specific tumor uptake; high hydrophilicity, with preferred renal excretion and low hepatobiliary excretion; and high stability but relatively rapid clearance from blood (6). Despite a large number of published derivatives, a valid comparison among them for the feasibility of tumor imaging is difficult because standardization between studies is lacking. Generally speaking, the majority of the radiotracers have relatively high renal and hepatic uptake, resulting in low tumor/liver and tumor/kidney ratios. In an effort to increase the tumor cell uptake and consequently improve the image contrast of tumors and their metastases, Santos-Cuevas et al. developed a hybrid peptide radiotracer (^99m^Tc-Tat-BN) and compared it with the GRPR agonist ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=HYNICBN99mTc) for the in vitro and in vivo uptake kinetics in GRPR-expressing cancer cells and tumor xenografts (1, 22). ^99m^Tc-Tat-BN was constructed by linking the HIV Tat-derived peptide (Tat(49-57)) with the GRPR agonist Lys^3^-BN peptide. Tat(49-57) is a small basic peptide with a sequence of H-Arg-Lys-Lys-Arg-Arg-Gln-Arg-Arg-Arg-NH_2_, and it has been successfully used for delivering a large variety of cargoes into cells because of its cell-penetrating properties (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=N2S2-Tat(49–57)-bombesin)]

The N_2_S_2_-Tat(49–57)-Lys^3^-BN hybrid peptide was synthesized by Santos-Cuevas et al. (1). It was composed of three components: Tat(49-57), a spacer sequence (Gly-Gly-Cys-Gly-Cys(acetamidomethyl group, Acm)-Gly-Cys(Acm)-NH_2_), and Lys^3^-BN. The Tat(49-57) peptide was used in an attempt to enhance the cell-penetrating capability of the hybrid peptide. The spacer was added for use as the specific N_2_S_2_-chelating site for ^99m^Tc. Briefly, Tat(49-57) peptide was first conjugated with the spacer to produce the Tat(49-57)-spacer-N_2_S_2_ peptide (H-Arg^1^-Lys^2^-Lys^3^-Arg^4^-Arg^5^-Gln^6^-Arg^7^-Arg^8^-Arg^9^-Gly^10^-Gly^11^-Cys^12^-Gly^13^-Cys^14^(Acm)-Gly^15^-Cys^16^(Acm)-NH_2_), and Lys^3^-BN peptide was conjugated with maleimidopropyl (MPA) through the Lys^3^ to create a branch with MPA group (Lys^3^-BN-MAP). The two peptides, Tat(49-57)-spacer-N_2_S_2_ and Lys^3^-BN-MAP, were then linked together by forming a thioether of the MPA group with the Cys^12^ side chain of the Tat(49-57)-spacer-N_2_S_2_ peptide (Tat-BN). The chemical purity of the hybrid peptide was >90% with a molecular weight of 3,779.5 g/mol. Radiolabeling was accomplished by a step of deprotection of the Acm groups, followed by sodium ^99m^Tc-pertechnetate reduction with stannous chloride in the presence of ammonium acetate and sodium tartrate at room temperature. The radioconjugate ^99m^Tc-Tat-BN remained stable after 24 h without post-labeling purification. The mean radiochemical purity was 92 ± 2% (n > 30), and the average specific activity was 14 MBq/nmol (0.38 mCi/nmol). The ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=HYNICBN99mTc) was synthesized as reported previously (22).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=N2S2-Tat(49–57)-bombesin)]

Santos-Cuevas et al. first estimated the stability of ^99m^Tc-Tat-BN in fresh human serum and the instability towards cysteine challenge (1). After incubation for 1 h at 37ºC with human serum, the radiochemical purity of ^99m^Tc-Tat-BN remained >90% and decreased to 82% and 65% after 3 h and 24 h, respectively. Protein binding was 36.4 ± 2.7% at 2 h. After incubation for 1 h at 5:1, 50:1, and 500:1 molar ratios of cysteine to ^99m^Tc-Tat-BN, the radioactivity dissociated from ^99m^Tc-Tat-BN was 7%, 16%, and 41%, respectively, indicating adequate stability towards cysteine.

Santos-Cuevas et al. then analyzed the in vitro uptake of ^99m^Tc-Tat-BN in PC-3, MDA-MB231, and MCF7 cells after incubation of the tumor cells with ^99m^Tc-Tat-BN or ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN at 37ºC for various times (1). The results showed that the tumor cell uptake was significantly higher for ^99m^Tc-Tat-BN than for ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN (P < 0.05) in all three cell lines. The maximum cell uptake was reached in PC-3 and MCF7 cells for both radiotracers between 2 and 4 h after incubation. However, MDA-MB231 cells showed a distinct pattern where cellular uptake reached a maximum during the first few minutes. For ^99m^Tc-Tat-BN, the maximum cell uptake (% of total activity) was 28.10 ± 3.86% in PC-3 cells at 4 h, 18.27 ± 2.14% in MCF7 cells at 2 h, and 24.33 ± 2.82% in MDA-MB231 cells at 5 min, respectively. For ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN, the maximum cell uptake was 17.62 ± 1.86% in PC-3 cells at 4 h, 8.97 ± 0.92% in MCF7 cells at 2 h, and 5.91 ± 0.26% in MDA-MB231 cells at 5 min, respectively. Most of the ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN remained on the cell membrane, while ^99m^Tc-Tat-BN was released in the cytoplasm, with a significant difference for the internalization between them (P < 0.05). Blocking studies showed that the tumor cell uptake for both radiotracers was inhibited by pre-incubation with cold BN (Lys^3^-BN). In general, cell binding in blocked cells was <3% of total activity for ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN and <9% for ^99m^Tc-Tat-BN in all three cell lines and for all time points examined (detailed data not shown).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=N2S2-Tat(49–57)-bombesin)]

Biodistribution of the ^99m^Tc-Tat-BN was studied in healthy 6-week-old Balb-C mice (n = 15) (1). Mice were given 1.11 MBq (30 µCi) ^99m^Tc-Tat-BN via tail vein, and they were euthanized at 0.25, 0.5, 2, 4, and 24 h after injection (n = 3 mice/time point). Among organs examined, the kidney had the highest radioactivity levels at all time points: 16.87 ± 4.85, 22.99 ± 8.57, 29.02 ± 2.78, 27.72 ± 2.18, and 8.45 ± 0.81% injected dose per gram of tissue (ID/g) at 0.25, 0.5, 2, 4, and 24 h after injection, respectively, indicating predominant renal excretion of the ^99m^Tc-Tat-BN. The radioactivity levels in the liver and intestine, although relatively low, also suggested the presence of hepatobiliary clearance. The pancreas, an organ with GRPR expression, also showed high uptake, and the radioactivity level was higher in the pancreas, than in non-excretory organs such as spleen, muscle, and even lung. No blocking studies were carried out.

Tumor xenograft uptake studies and imaging were performed on athymic male mice bearing subcutaneous PC-3 tumor xenografts (1). Mice were given 3 MBq (0.08 mCi) ^99m^Tc-Tat-BN or ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN via tail vein (n = 3 mice/radiotracer), and they were euthanized at 2 h after injection. The tumor/blood, tumor/muscle, and pancreas/blood ratios were 4.4, 7, and 8.2, respectively, for ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN, and 3.2, 8, and 1.4, for ^99m^Tc-Tat-BN, respectively. In vivo and ex vivo imaging showed a clear tumor uptake of both ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN and ^99m^Tc-Tat-BN. The tumor/muscle ratio obtained from image counts per pixel was 7 for ^99m^Tc-EDDA/HYNIC-[Lys^3^]-BN and 8.5 for ^99m^Tc-Tat-BN, indicating a minimal difference between the two radiotracers. No blocking studies were carried out.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Santos-Cuevas C.L., Ferro-Flores G., Arteaga de Murphy C., Ramirez Fde M., Luna-Gutierrez M.A., Pedraza-Lopez M., Garcia-Becerra R., Ordaz-Rosado D. (2009). Design, preparation, in vitro and in vivo evaluation of (99m)Tc-N2S2-Tat(49-57)-bombesin: a target-specific hybrid radiopharmaceutical. Int J Pharm.
2 Maina T., Nock B.A., Zhang H., Nikolopoulou A., Waser B., Reubi J.C., Maecke H.R. (2005). Species differences of bombesin analog interactions with GRP-R define the choice of animal models in the development of GRP-R-targeting drugs. J Nucl Med.
3 Smith C.J., Volkert W.A., Hoffman T.J. (2003). Gastrin releasing peptide (GRP) receptor targeted radiopharmaceuticals: a concise update. Nucl Med Biol.
4 Erspamer V., Erpamer G.F., Inselvini M. (1970). Some pharmacological actions of alytesin and bombesin. J Pharm Pharmacol.
5 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
6 Ananias H.J., de Jong I.J., Dierckx R.A., van de Wiele C., Helfrich W., Elsinga P.H. (2008). Nuclear imaging of prostate cancer with gastrin-releasing-peptide-receptor targeted radiopharmaceuticals. Curr Pharm Des.
7 Ischia J., Patel O., Shulkes A., Baldwin G.S. (2009). Gastrin-releasing peptide: different forms, different functions. Biofactors.
8 Maina T., Nock B., Mather S. (2006). Targeting prostate cancer with radiolabelled bombesins. Cancer Imaging.
9 Weber H.C. (2009). Regulation and signaling of human bombesin receptors and their biological effects. Curr Opin Endocrinol Diabetes Obes.
10 Yang Y.S., Zhang X., Xiong Z., Chen X. (2006). Comparative in vitro and in vivo evaluation of two 64Cu-labeled bombesin analogs in a mouse model of human prostate adenocarcinoma. Nucl Med Biol.
11 Liu S., Edwards D.S., Barrett J.A. (1997). 99mTc labeling of highly potent small peptides. Bioconjug Chem.
12 Zhang X., Cai W., Cao F., Schreibmann E., Wu Y., Wu J.C., Xing L., Chen X. (2006). 18F-labeled bombesin analogs for targeting GRP receptor-expressing prostate cancer. J Nucl Med.
13 Schroeder R.P., van Weerden W.M., Bangma C., Krenning E.P., de Jong M. (2009). Peptide receptor imaging of prostate cancer with radiolabelled bombesin analogues. Methods.
14 Chen X., Park R., Hou Y., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). microPET and autoradiographic imaging of GRP receptor expression with 64Cu-DOTA-[Lys3]bombesin in human prostate adenocarcinoma xenografts. J Nucl Med.
15 Hohne A., Mu L., Honer M., Schubiger P.A., Ametamey S.M., Graham K., Stellfeld T., Borkowski S., Berndorff D., Klar U., Voigtmann U., Cyr J.E., Friebe M., Dinkelborg L., Srinivasan A. (2008). Synthesis, 18F-labeling, and in vitro and in vivo studies of bombesin peptides modified with silicon-based building blocks. Bioconjug Chem.
16 Li Z.B., Wu Z., Chen K., Ryu E.K., Chen X. (2008). 18F-labeled BBN-RGD heterodimer for prostate cancer imaging. J Nucl Med.
17 Prasanphanich A.F., Retzloff L., Lane S.R., Nanda P.K., Sieckman G.L., Rold T.L., Ma L., Figueroa S.D., Sublett S.V., Hoffman T.J., Smith C.J. (2009). In vitro and in vivo analysis of [(64)Cu-NO2A-8-Aoc-BBN(7-14)NH(2)]: a site-directed radiopharmaceutical for positron-emission tomography imaging of T-47D human breast cancer tumors. Nucl Med Biol.
18 Fragogeorgi E.A., Zikos C., Gourni E., Bouziotis P., Paravatou-Petsotas M., Loudos G., Mitsokapas N., Xanthopoulos S., Mavri-Vavayanni M., Livaniou E., Varvarigou A.D., Archimandritis S.C. (2009). Spacer Site Modifications for the Improvement of the in Vitro and in Vivo Binding Properties of (99m)Tc-N(3)S-X-Bombesin[2-14] Derivatives. Bioconjug Chem.
19 Nock B., Nikolopoulou A., Chiotellis E., Loudos G., Maintas D., Reubi J.C., Maina T. (2003). [99mTc]Demobesin 1, a novel potent bombesin analogue for GRP receptor-targeted tumour imaging. Eur J Nucl Med Mol Imaging.
20 Cescato R., Maina T., Nock B., Nikolopoulou A., Charalambidis D., Piccand V., Reubi J.C. (2008). Bombesin receptor antagonists may be preferable to agonists for tumor targeting. J Nucl Med.
21 Nock B.A., Nikolopoulou A., Galanis A., Cordopatis P., Waser B., Reubi J.C., Maina T. (2005). Potent bombesin-like peptides for GRP-receptor targeting of tumors with 99mTc: a preclinical study. J Med Chem.
22 Ferro-Flores G., Arteaga de Murphy C., Rodriguez-Cortes J., Pedraza-Lopez M., Ramirez-Iglesias M.T. (2006). Preparation and evaluation of 99mTc-EDDA/HYNIC-[Lys 3]-bombesin for imaging gastrin-releasing peptide receptor-positive tumours. Nucl Med Commun.